# ^64^Cu-1,4,7,10-Tetraazacyclododecane-1,4,7,10-tetraacetic acid-Arg-rich Cys knot scaffold grafted with integrin α_v_β_6_-binding peptide RSLARTDLDHLRGR

Chemical name: | 64Cu-1,4,7,10-Tetraazacyclododecane-1,4,7,10-tetraacetic acid-Arg-rich Cys Knot scaffolds grafted with integrin α_v_β_6-_binding peptide RSLARTDLDHLRGR
Abbreviated name: | ^64^Cu-DOTA-R_0_1
Synonym:
Backbone: | Peptide
Target: | Integrin α_v_β_6_
Mechanism: | Receptor binding
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=arginine%20knot)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. α_v_β_3_ antagonists are being studied as antitumor and antiangiogenic agents, and the agonists are being studied as angiogenic agents for coronary angiogenesis (6, 8, 9). A tripeptide sequence consisting of Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_ and α_v_β_6_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (10).

Integrin α_v_β_6_ plays an important role in the development of epithelial cells and is nearly undetectable on adult normal tissues. However, the levels of α_v_β_6_ integrin can be upregulated during tissue remodeling and wound healing (11). On the other hand, α_v_β_6_ integrin is strongly expressed on tumor cells of the oral cavity, pancreas, breast, ovary, colon, and stomach (12-14). α_v_β_6_ integrin affects tumor growth, tumor invasiveness, and metastasis (13). α_v_β_6_ binds to the RGD motif in fibronectin, tenascin, and the viral protein 1 (VP1) of foot-and-mouth disease virus (FMDV) (15). FMDV binds to cells through the RGD motif of the GH loop of the VP1. A consensus α_v_β_6_-binding motif DLXXL was identified by using phage display screening with minimal binding to α_v_β_3_, α_IIb_β_3_, and α_v_β_5_ (16). Engineered cysteine knot peptides (knots) comprise a rigid molecular scaffold of ~4 kDa with three disulfide bonds and a centrally located β sheet. Kimura et al. (17) grafted a α_v_β_6_-binding peptide (RSLARTDLDHLRGR) into the loop 1 of an Arg-rich knot to produce the knot known as R_0_1, which was radiolabeled with ^64^Cu via 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA) conjugation to form ^64^Cu-DOTA-R_0_1 as a positron emission tomography (PET) probe for in vivo imaging of α_v_β_6_ integrin in tumor-bearing nude mice.

### Related Resource Links:

- Chapters in MICAD (Knot peptide (http://www.ncbi.nlm.nih.gov/books?term=knot%20AND%20micad%5Bbook%5D), RGD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=RGD+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), β_6_ integrin (http://www.ncbi.nlm.nih.gov/gene/3694))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), β_6_ integrin (http://www.ncbi.nlm.nih.gov/omim/147558))
- Clinical trials (RGD (http://www.clinicaltrials.gov/ct2/results?term=RGD))
- Drug information in FDA (RGD (http://google2.fda.gov/search?q=RGD&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=arginine%20knot%20and%20synthesis)]

Kimura et al. (17) reported the synthesis of ^64^Cu-DOTA-R_0_1. R_0_1 was synthesized and folded. The N-terminus amine of R_0_1 was conjugated with DOTA-N-hydroxysuccinimide ester for labeling with ^64^Cu. The radiochemical purity was >95%, with a specific activity of 18.5 MBq/nmol (0.5 mCi/nmol) at the end of high-performance liquid chromatography purification. The labeling yield was >80%. Molecular masses of R_0_1 (3.911 kDa) and DOTA-R_0_1 (4.293 kDa) were confirmed with matrix-assisted laser desorption/ionization-mass spectrometry. ^64^Cu-DOTA-R_0_1 remained >80% intact in mouse serum for 24 h at 37°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=arginine%20knot%20and%20%28in%20vitro%20or%20cell%29)]

Competitive binding of soluble integrins α_v_β_6,_ α_v_β_3_, α_v_β_5,_ and α_5_β_1_ to yeast cells expressing R_0_1 was determined with flow cytometry (17). The binding affinity (K_d_) value for α_v_β_6_ was 3.6 ± 0.9 nM. Integrins α_v_β_3_, α_v_β_5,_ and α_5_β_1_ (10-300 nM) exhibited little binding to R_0_1. Cellular accumulation of ^64^Cu-DOTA-R_0_1 was determined in A431 human epidermoid cancer and BxPC3 human pancreatic cancer cells (high α_v_β_6_-expression), and HEK293 human embryonic kidney cells (low α_v_β_6_-expression). A431 and BxPC3 cells exhibited one-fold higher radioactivity than that of HEK293 cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=arginine%20knot%20and%20rodentia)]

Kimura et al. (17) performed biodistribution studies with 3.7 MBq (0.1 mCi, 0.15 nmol) ^64^Cu-DOTA-R_0_1 in nude mice (n = 3/group) bearing BxPC3 xenografts. Data were obtained at 1 and 24 h after injection. ^64^Cu-DOTA-R_0_1 had blood levels of 0.46 and 0.52% (injected dose (ID)/g) at 1 and 24 h. The initial tracer accumulation in the α_v_β_6_-integrin-expressing BxPC3 tumor was about 4.13% ID/g at 1 h and decreased to 3.31% ID/g at 24 h. At 60 min, the highest radioactivity concentration was found in the kidney (68% ID/g), followed by the lung (2.78% ID/g), stomach (2.31% ID/g), liver (2.28% ID/g), and intestine (1.49% ID/g). The spleen, bone, muscle, skin, pancreas and heart showed low levels of radioactivity (<1% ID/g). The tumor/muscle ratios were 8.89 and 6.52 at 1 and 24 h, respectively. No blocking studies were performed.

^64^Cu-DOTA-R_0_1 PET imaging studies were performed in nude mice (n = 3) bearing both BxPC3 and HEK293 xenografts at 1, 2, 4, and 24 h after injection of 3.7 MBq (0.1 mCi, 0.15 nmol) ^64^Cu-DOTA-R_0_1 (17). The BxPC3 tumors were clearly visualized as early as 1 h and as late as 24 h after injection. Major radioactivity was observed in the urinary bladder and kidneys. Region of interest analysis showed the tumor accumulation of ^64^Cu-DOTA-S_0_2 was ~3.5% ID/g in BxPC3 tumors compared with ~1% ID/g in HEK293 tumors. Average tumor/background ratios were ~7 (BxPC3) and ~2 (HEK293). No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=arginine%20knot%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=arginine%20knot%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=arginine%20knot%20and%20%28human%20not%20cell%29)]

No publication is currently available.

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Breuss J.M., Gallo J., DeLisser H.M., Klimanskaya I.V., Folkesson H.G., Pittet J.F., Nishimura S.L., Aldape K., Landers D.V., Carpenter W., et al. (1995). Expression of the beta 6 integrin subunit in development, neoplasia and tissue repair suggests a role in epithelial remodeling. J Cell Sci.
12 Thomas G.J., Nystrom M.L., Marshall J.F. (2006). Alphavbeta6 integrin in wound healing and cancer of the oral cavity. J Oral Pathol Med.
13 Kawashima A., Tsugawa S., Boku A., Kobayashi M., Minamoto T., Nakanishi I., Oda Y. (2003). Expression of alphav integrin family in gastric carcinomas: increased alphavbeta6 is associated with lymph node metastasis. Pathol Res Pract.
14 Bates R.C. (2005). The alphaVbeta6 integrin as a novel molecular target for colorectal cancer. Future Oncol.
15 DiCara D., Rapisarda C., Sutcliffe J.L., Violette S.M., Weinreb P.H., Hart I.R., Howard M.J., Marshall J.F. (2007). Structure-function analysis of Arg-Gly-Asp helix motifs in alpha v beta 6 integrin ligands. J Biol Chem.
16 Kraft S., Diefenbach B., Mehta R., Jonczyk A., Luckenbach G.A., Goodman S.L. (1999). Definition of an unexpected ligand recognition motif for alphav beta6 integrin. J Biol Chem.
17 Kimura R.H., Teed R., Hackel B.J., Pysz M.A., Chuang C.Z., Sathirachinda A., Willmann J.K., Gambhir S.S. (2012). Pharmacokinetically stabilized cystine knot peptides that bind alpha-v-beta-6 integrin with single-digit nanomolar affinities for detection of pancreatic cancer. Clin Cancer Res.